# ^99m^Tc-Diethylenetriaminepentaacetate-deoxyglucose

Chemical name: | ^99m^Tc-Diethylenetriaminepentaacetate-deoxyglucose
Abbreviated name: | ^99m^Tc-DTPA-DG
Synonym: | ^99m^Tc-Deoxyglucose
Agent Category: | Compound
Target: | Glucose transporter and hexokinases
Target Category: | Specific binding and phosphorylation
Method of detection: | Single-Photon Emission Computed Tomography (SPECT) , Planar gamma imaging
Source of signal /contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29)]

^99m^Tc-diethylenetriaminepentaacetate-deoxyglucose (^99m^Tc-DTPA-DG) is a radioligand developed for single-photon emission computed tomography (SPECT) of glucose utilization rates in normal and pathologic diseases that reflect tumor cell proliferation activities and viability (1). ^99m^Tc is a gamma emitter with a physical half-life (t_½_) of 6.02 h.

Movement of glucose into and out of cells is mediated by one or more members of the transport protein family of glucose transporters (2). There are different classes of glucose transporters for two forms of glucose transport. SGLT1 and SGLT2 are sodium glucose cotransporters involved in secondary active transport, and GLUT1 to GLUT13 are facilitated glucose transporters (3). They are similar in that they have a polypeptide chain of 500 amino acids. After glucose enters a living cell, phosphorylation catalyzed by hexokinase transforms the molecule to glucose-6-phosphate (G-6-P). There are four hexokinase isoforms (HKI to HKIV) that exist in mammalian tissues (4). The G-6-P isomerase then converts G-6-P into fructose-6-phosphate (F-6-P) by rearranging the carbonyl group from the C-1 to the C-2 position in the ring structure to enter further metabolic pathways. Cancer cells are known to have accelerated metabolism, high glucose consumption, and increased glucose uptake (5). In humans, high levels of GLUT expression in tumors have been associated with poor survival. Increased HK activities have also been associated with metastatic disease.

Molecular imaging with glucose analogs is a useful tool in the detection, staging, and therapy response monitoring of various malignant neoplasms (6, 7). 2-[^18^F]Fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) was the first successful radiolabeled glucose analog developed for clinical positron emission tomography (PET) applications (8). [^18^F]FDG, like glucose, is transported into cells by glucose transporters and is a substrate for hexokinase. However, it is converted to [^18^F]FDG-6-phosphate ([^18^F]FDG-6-P), which cannot be further metabolized. [^18^F]FDG-6-P is not a substrate for the G-6-P isomerase and therefore is metabolically trapped in the cell. The trapping of [^18^F]FDG-6-P within cells and tissues allows in vivo PET imaging of glucose utilization rates in normal and pathologic tissues. Because of the short t_½_ of ^18^F and the requirement of cyclotron production, it is desirable to develop a gamma-emitter for SPECT imaging (9). Early ^123^I-labeled glucose analogs were either chemically unstable or poor substrates for hexokinase (6, 10, 11). Bayly et al. (12) reported the successful synthesis of a glucosamine labeled with the tricarbonyls of ^99m^Tc(I). Yang et al. (13, 14) also demonstrated the feasibility of synthesis and imaging of ^99m^Tc-ethylenedicysteine-deoxyglucose in rodents bearing tumors. These studies did not attempt to determine whether these glucose analogs actually followed the key steps in glucose metabolism. Chen et al. (1) developed a one-step ^99m^Tc-DTPA-DG kit and showed tumor accumulation of ^99m^Tc-DTPA-DG in nude rats bearing MCF-7 human mammary tumors. However, the mechanism of tumor uptake was not investigated.

## Synthesis

[PubMKed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20synthesis)]

Chen et al. (1) reported the synthesis of ^99m^Tc-DTPA-DG from commercially available D-glucosamine hydrochloride. Briefly, thionyl chloride was first added dropwise to DTPA with stirring at 0ºC. The mixture was then continuously stirred in boiling water for 3 h and refluxed for 20 h. The mixture was distilled to remove excess thionyl chloride, and then dianhydride acylchloride, dimethyl sulfoxide, pyridine, and D-glucosamine hydrochloride were added. The reaction mixture was stirred in a boiling water bath for 24–48 h. DTPA-DG was isolated by dialysis or gel chromatography. Radiolabeling with ^99m^Tc was performed by first preparing DTPA-DG reaction kits that contained 25 mg DTPA-DG and 0.5 mg stannous chloride. The pH was adjusted to 6.0. The shelf life of the kit lasted at least 3 months at 4ºC. At the time of radiolabeling, ~200−300 MBq (5.4−8.1 mCi) ^99m^Tc pertechnetate was added to each kit, gently mixed, and incubated at room temperature for 30 min. The radiochemical purity was 99.2% at 30 min and remained >98.6% after 6 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20in%20vitro)]

In vitro cellular uptake assay of ^99m^Tc-DTPA-DG was performed with the MCD-7 cell line, with ^99m^Tc-DTPA and [^18^F]FDG serving as the controls (1). Both ^99m^Tc-DTPA-DG and [^18^F]FDG had significantly increased radioactivity localized in the cancer cells when compared with ^99m^Tc-DTPA (P<0.05). At 4 h after incubation, 0.5% of ^99m^Tc-DTPA-DG radioactivity was localized in the cells. In comparison, >0.6% [^18^F]FDG radioactivity was taken up by the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20rodentia)]

Chen et al. (1) injected 0.037−0.111 MBq (1−3 μCi) ^99m^Tc-DTPA-DG intravenously into nude rats bearing MCF-7 tumors (right leg muscle ~6 mm in diameter) for biodistribution studies. ^99m^Tc-DTPA-DG was rapidly cleared from the blood and excreted by the kidneys. The tumor radioactivity levels (n = 3) were 5.12 ± 1.43 (10 min), 3.10 ± 0.87 (1 h), 2.10 ± 0.02 (2 h), 1.59 ± 0.04 (4 h), and 1.69 ± 0.03 (8 h). The tumor/blood ratios were 0.45 ± 0.09 (10 min), 1.29 ± 0.26 (1 h), 3.13 ± 0.63 (2 h), 3.24 ± 0.65 (4 h), and 3.38 ± 0.68 (8 h). The kidney radioactivity levels were 28.86 ± 8.88 (10 min), 10.63 ± 4.35 (1 h), 4.45 ± 0.98 (2 h), 4.22 ± 2.00 (4 h), and 1.99 ± 0.12 (8 h). The liver radioactivity levels were 5.20 ± 0.93 (10 min), 2.68 ± 0.32 (1 h), 2.76 ± 1.05 (2 h), 1.67 ± 0.29 (4 h), and 1.37 ± 0.47 (8 h). No significant radioactivity accumulation was found in other organs. In comparison, [^18^F]FDG had tumor radioactivity levels of 2.84 ± 1.03 (10 min), 1.43 ± 0.65 (2 h), and 1.42 ± 0.12 (4 h). The tumor/blood ratios of [^18^F]FDG were 1.58 ± 1.65 (10 min), 5.73 ± 2.78 (2 h), and 7.12 ± 2.12 (4 h).

Planar gamma imaging was conducted in nude rats bearing MCF-7 tumors. An i.v. dose of 11.1 MBq (0.3 mCi) ^99m^Tc-DTPA-DG was administered to each rat. There was a marked increase in tumor radioactivity that enabled good visualization of the tumors at 2 and 4 h. The region of interest (ROI) ratios for tumor/nontumor were 2.46 ± 1.02 and 3.54 ± 1.36 at 0.5 and 2 h, respectively. The kidneys, liver, and bladder were also visualized. Little radioactivity was observed in the thyroid gland and stomach, and the authors suggested that this indicated good in vivo stability of ^99m^Tc-DTPA-DG. In comparison, the tumor/nontumor ratios for ^99m^Tc-DTPA were 1.16 ± 0.02 and 1.14 ± 0.03 at 0.5 and 2 h, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-DTPA-DG%29%20OR%20%28technetium-99m-labeled%20deoxyglucose%29%29%20AND%20human)]

No publication is currently available.

## References

1 Chen Y., Huang Z.W., He L., Zheng S.L., Li J.L., Qin D.L. (2006). Synthesis and evaluation of a technetium-99m-labeled diethylenetriaminepentaacetate-deoxyglucose complex ([99mTc]-DTPA-DG) as a potential imaging modality for tumors. Appl Radiat Isot.
2 Brown G.K. (2000). Glucose transporters: structure, function and consequences of deficiency. J Inherit Metab Dis.
3 Pauwels E.K., Ribeiro M.J., Stoot J.H., McCready V.R., Bourguignon M., Maziere B. (1998). FDG accumulation and tumor biology. Nucl Med Biol.
4 Smith T.A. (2000). Mammalian hexokinases and their abnormal expression in cancer. Br J Biomed Sci.
5 Macheda M.L., Rogers S., Best J.D. (2005). Molecular and cellular regulation of glucose transporter (GLUT) proteins in cancer. J Cell Physiol.
6 Gatley S.J. (2003). Labeled glucose analogs in the genomic era. J Nucl Med.
7 Abouzied M.M., Crawford E.S., Nabi H.A. (2005). 18F-FDG imaging: pitfalls and artifacts. J Nucl Med Technol.
8 Fowler J.S., Ido T. (2002). Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
9 Chen X., Li L., Liu F., Liu B. (2006). Synthesis and biological evaluation of technetium-99m-labeled deoxyglucose derivatives as imaging agents for tumor. Bioorg Med Chem Lett.
10 Matte G., Adam M., Lyster D. (2001). Biological evaluation of 2-fluoro-2-[123I]iodo-mannose (FIM): biological evaluation of FIM. Nucl Med Biol.
11 Kloster G., Laufer P., Wutz W., Stocklin G. (1983). 75,77Br- and 123I-analogues of D-glucose as potential tracers for glucose utilisation in heart and brain. Eur J Nucl Med.
12 Bayly S.R., Fisher C.L., Storr T., Adam M.J., Orvig C. (2004). Carbohydrate conjugates for molecular imaging and radiotherapy: 99mTc(I) and 186Re(I) tricarbonyl complexes of N-(2'-Hydroxybenzyl)-2-amino-2-deoxy-D-glucose. Bioconjug Chem.
13 Yang D.J., Kim C.G., Schechter N.R., Azhdarinia A., Yu D.F., Oh C.S., Bryant J.L., Won J.J., Kim E.E., Podoloff D.A. (2003). Imaging with 99mTc ECDG targeted at the multifunctional glucose transport system: feasibility study with rodents. Radiology.
14 Yang D., Yukihiro M., Yu D.F., Ito M., Oh C.S., Kohanim S., Azhdarinia A., Kim C.G., Bryant J., Kim E.E., Podoloff D. (2004). Assessment of therapeutic tumor response using 99mtc-ethylenedicysteine-glucosamine. Cancer Biother Radiopharm.